# ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[c(Arg-Gly-Asp-D-Tyr-Lys)]_2_

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[c(Arg-Gly-Asp-D-Tyr-Lys)]_2_
Abbreviated name: | ^68^Ga-NOTA-RGD2, ^68^Ga-NOTA-E-[c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (50% inhibition concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides and peptidominetics have been found to have high accumulation in tumors in mice (12, 13). Out of these developments [^18^F]Galacto-c(RGDfK) has been evaluated in a number of clinical studies for imaging of α_v_β_3_ in cancer patients (14-19). Li et al. (20) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling Glu-[cyclo(RGDyK)]_2_ (RGD2) to form (^68^Ga-NOTA-RGD2) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing human glioblastoma U87MG tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+synthesis)]

RGD2 was prepared with solid-phase peptide synthesis (20). Addition of the NOTA group to RGD2 was performed by mixing 2 µmol RGD2 with 6 μmol S-2-(4-isothiocyanatobenzyl)-NOTA in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. NOTA-RGD2 was isolated with high-performance liquid chromatography (HPLC) with 52% yield. Molecular weight was determined with MALDI-TOF-MS to be m/z 1,800.2 Da (calculated molecular weight, 1,800.8 Da). For ^68^Ga labeling, a solution of 185 MBq (5 mCi) ^68^GaCl_3_ and 10 nmol RGD2 was heated for 10 min at 40°C. ^68^Ga-NOTA-RGD2 was purified with HPLC with a yield of 82% and a radiochemical purity of >98%. The specific activity was 9.7–13.6 MBq/nmol (0.26–0.37 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+in+vitro)]

Li et al. (20) performed in vitro inhibition studies of NOTA-RGD2 in cultured human U87MG cells with ^125^I-echistatin. The 50% inhibition concentration (IC_50_) values were 189, 218, 60, and 16 nM for c(RGDyK), NOTA-RGD1, NOTA-RGD2, and NOTA-RGD4, respectively. NOTA-RGD1 and c(RGDyK) had comparable IC_50_ values, indicating that NOTA conjugation had little effect on the receptor binding affinity. Due to the dual-binding valency effect, NOTA-RGD2 and NOTA-RGD4 had two-fold and 12-fold higher binding affinity than NOTA-RGD1, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+%20rodentia)]

Li et al. (20) performed ex vivo biodistribution studies of 3.7 MBq (100 μCi) ^68^Ga-NOTA-RGD2 in nude mice bearing U87MG xenografts at 1 h after injection. Tumor and kidney accumulation was 3.8 ± 0.7% and 4.3 ± 0.7% injected dose per gram (ID/g), whereas the accumulation values were ~1% ID/g or less in other tissues. The RGD2 dimer tracer exhibited a higher tumor accumulation than the RGD1 monomer tracer and lower background than the RGD4 tetramer tracer. Coinjection of excess c(RGDyK) (10 mg/kg) and ^68^Ga-NOTA-RGD2 inhibited the tumor accumulation by 95%, whereas the accumulation in the kidneys was inhibited by only 35%. Various small inhibitory effects were also observed in the other tissues and organs. PET imaging in nude mice bearing U87MG xenografts was performed with 3.7 MBq (0.1 mCi) ^68^Ga-NOTA-RGD2 for 2 h after injection. Quantitative analyses of PET imaging data showed that the radioactivity levels in the U87MG tumors (n = 3 mice) were 4.4% ID/g (5 min), 3.5% ID/g (15 min), 2.8% ID/g (30 min), 2.3% ID/g (60 min), and 1.9% ID/g (120 min). ^68^Ga-NOTA-RGD2 was excreted mainly through the kidneys. The tumor/muscle ratio was ~6 at 60 min after injection. Coinjection of c(RGDyK) and ^68^Ga-NOTA-RGD2 reduced the tumor accumulation to the background level at 60 min after injection. The radioactivity level in the liver, kidneys, and muscle was also reduced.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
13 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
14 Beer A.J., Grosu A.L., Carlsen J., Kolk A., Sarbia M., Stangier I., Watzlowik P., Wester H.J., Haubner R., Schwaiger M. (2007). [18F]galacto-RGD positron emission tomography for imaging of alphavbeta3 expression on the neovasculature in patients with squamous cell carcinoma of the head and neck. Clin Cancer Res.
15 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.
16 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
17 Beer A.J., Lorenzen S., Metz S., Herrmann K., Watzlowik P., Wester H.J., Peschel C., Lordick F., Schwaiger M. (2008). Comparison of integrin alphaVbeta3 expression and glucose metabolism in primary and metastatic lesions in cancer patients: a PET study using 18F-galacto-RGD and 18F-FDG. J Nucl Med.
18 Beer A.J., Niemeyer M., Carlsen J., Sarbia M., Nahrig J., Watzlowik P., Wester H.J., Harbeck N., Schwaiger M. (2008). Patterns of alphavbeta3 expression in primary and metastatic human breast cancer as shown by 18F-Galacto-RGD PET. J Nucl Med.
19 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
20 Li Z.B., Chen K., Chen X. (2008). (68)Ga-labeled multimeric RGD peptides for microPET imaging of integrin alpha(v)beta (3) expression. Eur J Nucl Med Mol Imaging.